# Ferumoxsil

Chemical name: | Ferumoxsil
Abbreviated name: | Large SPIO
Synonym: | Siloxane-coated SPIO, AMI-121
Agent Category: | Superparamagnetic Iron Oxide
Target: | Reticuloendothelial system
Target Category: | Internalized by phagocytes
Method of detection: | Magnetic Resonance imaging (MRI)
Source of signal/contrast: | Iron oxide
Activation: | No
Studies: | - In vitro; - Rodents; - Humans | No structure is available in PubChem (http://pubchem.ncbi.nlm.nih.gov).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22ferumoxsil%22%5BSubstance%20Name%5D)]

Magnetic resonance imaging (MRI) maps information about tissues spatially and functionally. Protons (hydrogen nuclei) are widely used to create images because of their abundance in water molecules. Water comprises about 80% of most soft tissues. The contrast of proton MRI depends mainly on the density of nuclear (proton spins), the relaxation times of the nuclear magnetization (T1, longitudinal and T2, transverse), the magnetic environment of the tissues, and the blood flow to the tissues. However, insufficient contrast between normal and diseased tissues requires development of contrast agents. Most of the contrast agents affect the T1 and T2 relaxation of the surrounding nuclei, mainly the protons of water. T-2* is the spin-spin relaxation time composed of variations from molecular interactions and intrinsic magnetic heterogeneities of tissues in the magnetic field [1].

Superparamagnetic iron oxide (SPIO) structure is composed of ferric iron (Fe^3+^) and ferrous iron (Fe^2+^) in the general formula of Fe_2_^3+^OFe^2+^O. The iron oxides particles are coated with a layer of dextran or other polysaccharide. These particles have a large combined magnetic moments or spins which are randomly rotated in the absence of an applied magnetic field. SPIO is used mainly as a T2 contrast agent in MRI though it can shorten both T1 and T2/T2* relaxation processes. SPIO particle uptake into reticuloendothelial system is by endocytosis or phagocytosis. SPIO particles are taken up by phagocytic cells such as monocytes, macrophages, and oligodendroglial cells. A variety of cells can also be labeled with these particles for cell trafficking and tumor-specific imaging studies. SPIO agents are classified by their sizes with coating material (about 20 nm to 3,500 nm in diameters) as large SPIO agents (Ferumoxsil or AMI-121, Ferucarbotran, OMP), standard SPIO (SSPIO) agents (Ferumoxides or AMI-25, SHU 555A), ultrasmall SPIO (USPIO) agents (Ferumoxtran or AMI-227, NC100150) and monocrystalline iron oxide nanoparticles (MION) agents [1].

Ferumoxsil is composed of iron particles of about 10 nm and the hydrodynamic diameter is about 300 nm. The iron particles are coated with a non-biodegradable and insoluble matrix (siloxane) and suspended in viscosity-increasing agents such as starch and cellulose [2]. They are used in oral large SPIO preparations. Ferumoxsil has been tested in clinical trials as negative contrast agent that decreases signal on T2 images. Ferumoxsil is used in bowel MR imaging.

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22ferumoxsil%22%5BSubstance%20Name%5D%20AND%20synthesis)]

SPIO agents are produced by controlling the precipitation of iron oxide in an aqueous solution of ferric salt, ferrous salt, and coating material by addition of an alkaline solution while active stirring or sonication is applied. The desired SPIO size of the agent is isolated and purified by differential centrifugation, column chromatography, and dialysis. Electron microscopy, X-ray diffraction and laser light scattering are used to measure median diameter of the nanoparticles. Relaxivities are measured by NMR spectroscopy [1].

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22ferumoxsil%22%5BSubstance%20Name%5D%20AND%20in%20vitro)]

No publication is currently available.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22ferumoxsil%22%5BSubstance%20Name%5D%20AND%20%28%22rodentia%22%5BMeSH%20Terms%5D%20OR%20rodentia%5BText%20Word%5D%29)]

Ferumoxsil preparations were well tolerated in rats without adverse effects as studied by hematological evaluations and histopathological examinations of organs and tissues. Most of ferumoxsil was eliminated in the feces by 72 hours. MRI of the rats showed that signal-intensity loss was detected without distortion artifacts [2].

## Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22ferumoxsil%22%5BSubstance%20Name%5D%20AND%20%28dog%20or%20pig%20or%20rabbit%20or%20sheep%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22ferumoxsil%22%5BSubstance%20Name%5D%20AND%20primates%20NOT%20humans)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22ferumoxsil%22%5BSubstance%20Name%5D%20AND%20humans)]

MRI with AMI-121 was performed in 15 volunteers. Loss of T2-weighted enhancement signal intensity was observed in the proximal and distal small bowel. Enhanced images showed improved marking of the head and tail of the pancreas, anterior regions of the kidneys, and para-arotic region [2]. AMI-121 MRI was helpful in discriminating normal bowel from solid lesions and in detecting subtle gastrointestinal tract mass change. In 30 consecutively studied patients suspected of having gastrointestinal pathology, oral contrast-enhanced computed tomography was more sensitive than AMI-121 MRI in detecting abdominal pathology. Conversely, AMI-121 MRI was more specific than computed tomography [3]. Oral ferumoxsil contrast agent is effective in gastrointestinal MR imaging and in delineation of normal and pathologic structures in the bowel [PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22ferumoxsil%22%5BSubstance%20Name%5D%20AND%20%22humans%22%5BMeSH%20Terms%5D%20AND%20%28%22intestines%22%5BMeSH%20Terms%5D%20OR%20bowel%5BText%20Word%5D%29)].

## References

1 Wang Y. X., Hussain S. M., Krestin G. P. (2001). Superparamagnetic iron oxide contrast agents: physicochemical characteristics and applications in MR imaging. Eur Radiol.
2 Hahn P. F., Stark D. D., Lewis J. M., Saini S., Elizondo G., Weissleder R., Fretz C. J., Ferrucci J. T. (1990). First clinical trial of a new superparamagnetic iron oxide for use as an oral gastrointestinal contrast agent in MR imaging. Radiology.
3 Johnson W. K., Stoupis C., Torres G. M., Rosenberg E. B., Ros P. R. (1996). Superparamagnetic iron oxide (SPIO) as an oral contrast agent in gastrointestinal (GI) magnetic resonance imaging (MRI): comparison with state-of-the-art computed tomography (CT). Magn Reson Imaging.